# ^111^In-CHX-A''-DTPA-anti-mindin/RG-1 monoclonal antibody 19G9

Chemical name: | ^111^In-CHX-A''-DTPA-anti-mindin/RG-1 monoclonal antibody 19G9
Abbreviated name: | ^111^In-CHX-A''-DTPA-19G9
Synonym:
Agent category: | Antibody
Target: | Mindin/RG-1 extracellular matrix protein
Target category: | Antigen, extracellular matrix protein
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=110347423), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=20987842) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=10418) for more information about mindin/RG-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9)]

Extracellular matrix (ECM) adhesion proteins consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Mindins are members of the mindin/F-spondin family of secreted ECM proteins (4). A human mindin homolog, mindin/RG-1, is expressed selectively in prostate tissues, and its expression level is elevated in some prostate tumors (5). Mindin/RG-1 protein expression is maintained in >80% of prostate cancers metastatic to bone or lymph nodes as well as in locally recurrent tumors in androgen-unresponsive patients. Furthermore, mindin/RG-1 expression in other normal tissues is lower than that expressed in the prostate. The fully humanized monoclonal antibody (mAb) 19G9 was generated against the mindin/RG-1 protein. Conjugation of mAb 19G9 with the bifunctional chelator [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans(S,S)-cyclohexane-1,2-diethylene triamine-pentaacetic acid (CHX-A''-DTPA) produced CHX-A''-DTPA-19G9, which was used for ^111^In labeling (5). ^111^In-CHX-A''-DTPA-19G9 has been evaluated in nude mice bearing human LNCaP tumor xenografts (5, 6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20synthesis)]

19G9 was incubated with CHX-A''-DTPA at a 1:50 molar ratio in sodium bicarbonate buffer (pH 8.5) for 18 h at room temperature (6). CHX-A''-DTPA-19G9 was isolated with column chromatography. CHX-A''-DTPA-19G9 was mixed with 5.6 MBq/nmol (0.15 mCi/nmol) ^111^InCl_3_ and incubated for 60 min. ^111^In-CHX-A''-DTPA-19G9 was isolated with column chromatography. The labeling efficiency of ^111^In incorporation was >98%. Specific activity of the preparation was 2.7 MBq/nmol (0.073 mCi/nmol). The number of CHX-A''-DTPA molecules per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20in%20vitro)]

Schneider et al. (6) performed binding experiments with 19G9 with the use of a Biacore sensor chip immobilized with mindin/RG-1 protein. The dissociation constant value of 19G9 was calculated to be 1.2 nM. Parry et al. (5) reported that the immunoreactivity of the antibody was maintained after CHX-A''-DTPA conjugation and after radiolabeling (data not shown).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20rodentia)]

Parry et al. (5) performed ex vivo biodistribution studies of ^111^In-CHX-A''-DTPA-19G9 in nude mice bearing human LNCaP xenografts (n = 3 mice/group). Initial tracer accumulation in the LNCaP tumors was 17% injected dose per gram (% ID/g) at 1 d, 22% ID/g at 3 d, 24% ID/g at 6 d, and 29% ID/g at 9 d after injection. The radioactivity level was higher in tumors than in other organs and tissues at these time points. The organ with the highest accumulation at 3 d after injection was the spleen (13.3% ID/g), followed by the liver (5.1% ID/g), kidney (4.8% ID/g), and lung (3.5% ID/g). Blood levels were ~5–7% ID/g at 3–9 d. Tumor/blood ratios were 1.2, 3.2, 4.4, and 5.2 at 1, 3, 6, and 9 d after injection, respectively. In contrast, ^111^In-CHX-A''-DTPA-IgG as a negative control showed only 7–8% ID/g in the tumors at these time points. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=19G9%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Feinstein Y., Klar A. (2004). The neuronal class 2 TSR proteins F-spondin and Mindin: a small family with divergent biological activities. Int J Biochem Cell Biol.
5 Parry R., Schneider D., Hudson D., Parkes D., Xuan J.A., Newton A., Toy P., Lin R., Harkins R., Alicke B., Biroc S., Kretschmer P.J., Halks-Miller M., Klocker H., Zhu Y., Larsen B., Cobb R.R., Bringmann P., Roth G., Lewis J.S., Dinter H., Parry G. (2005). Identification of a novel prostate tumor target, mindin/RG-1, for antibody-based radiotherapy of prostate cancer. Cancer Res.
6 Schneider D.W., Heitner T., Alicke B., Light D.R., McLean K., Satozawa N., Parry G., Yoo J., Lewis J.S., Parry R. (2009). In vivo biodistribution, PET imaging, and tumor accumulation of 86Y- and 111In-antimindin/RG-1, engineered antibody fragments in LNCaP tumor-bearing nude mice. J Nucl Med.